# 2-(4-Aminophenyl)-6-(2-([^18^F]fluoroethoxy))quinoline

Chemical name: | 2-(4-Aminophenyl)-6-(2-([^18^F]fluoroethoxy))quinoline
Abbreviated name: | [^18^F]THK523
Synonym:
Agent category: | Compound
Target: | Tau fibrils
Target category: | Acceptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=THK523)]

Alzheimer's disease (AD) is a form of dementia with a gradual memory loss and a progressive decline in mental functions over time (1, 2). It is characterized pathologically by neuronal loss, extracellular senile plaques (aggregates of amyloid-β peptides consisting of 40–42 amino acids), and intracellular neurofibrillary tangles (filaments of microtubule-binding hyper-phosphorylated protein tau) in the brain, especially in the hippocampus and associative regions of the cortex (3, 4). β-Amyloid fibrils and tau neurofibrillary tangles are implicated as the main causes of neuronal degeneration and cell death (5, 6).

Early diagnosis of AD is important for treatment consideration and disease management (7). Various β-amyloid imaging agents have been developed for magnetic resonance imaging, single-photon emission computed tomography, and positron emission tomography (PET) (8-13). The binding properties of different derivatives of Congo red, thioflavin, stibene, and aminonaphthalene have been studied in post-mortem human brain tissue and in transgenic mice. Of these analogs, 2-(1-(6-[(2-[^18^F]fluoroethyl)(methyl)amino]-2-naphthyl)ethylidene)malono nitrile ([^18^F]FDDNP) has been studied in humans, showing more binding in the brains of patients with AD than in those of healthy people (14). [^18^F]FDDNP has been found to bind to both β-amyloid fibrils and tau neurofibrillary tangles. However, [^18^F]FDDNP showed low signal/noise ratios for PET imaging because it is highly lipophilic. N-methyl-[^11^C]-2-(4’-methylaminophenyl)-6-hydroxybenzothiasole, a β-amyloid binding compound based on a series of neutral thioflavin-T derivatives, was radiolabeled with the positron-emitting radionuclide ^11^C ([^11^C]6-OH-BTA-1 or [^11^C]PIB). [^11^C]6-OH-BTA-1 was found to be a promising imaging agent for β-amyloid fibrils in the brain (10). Okamura et al. (15) identified a series of quinolone derivatives that bind tau neurofibrillary tangles with higher affinity than β-amyloid fibrils. One of these derivatives, 2-(4-aminophenyl)-6-(2-([^18^F]fluoroethoxy))quinolone ([^18^F]THK523), has been evaluated for imaging of tau pathology in the brain (16).

### Related Resource Links:

- Chapters in MICAD (Amyloid (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=amyloid+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), tau (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=tau+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Amyloid (http://www.ncbi.nlm.nih.gov/gene/351), tau (http://www.ncbi.nlm.nih.gov/gene/4137)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (Amyloid (http://www.ncbi.nlm.nih.gov/omim/104760), tau (http://www.ncbi.nlm.nih.gov/omim/157140))
- Clinical trials (Amyloid (http://www.clinicaltrials.gov/ct2/results?term=Amyloid), tau (http://www.clinicaltrials.gov/ct2/results?term=tau+imaging))
- Drug information in FDA (Amyloid inhibitors (http://google2.fda.gov/search?q=Amyloid+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=16&y=16), tau inhibitors (http://google2.fda.gov/search?q=tau+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=7))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=THK523%20and%20synthesis)]

[^18^F]THK523 was readily synthesized by standard ^18^F-fluorination of the tosylate precursor ([^18^F]KF/Kryptofix2.2.2, 10 min at 110°C) (16). [^18^F]THK523 was purified with high-performance liquid chromatography. Overall yield was 24%, with a specific activity of 100 GBq/µmol (2.7 Ci/µmol) at the end of synthesis and a radiochemical purity of >95%. Total synthesis time was not reported. The LogP_oct_ (lipophilicity) value was measured to be 2.91 ± 0.13 (n = 3).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=THK523%20and%20in%20vitro)]

Fodero-Tavoletti et al. (16) performed saturation binding studies of [^18^F]THK523 with β-amyloid(1-40) fibrils and human recombinant K18Δ280K-tau fibrils in the presence of excess THK523. [^18^F]THK523 exhibited two binding sites on K18Δ280K-tau fibrils, with K_d1_ and K_d2_ values of 1.67 nM and 21.74 nM, respectively. On the other hand, only one [^18^F]THK523 binding site was identified on β-amyloid(1-40) fibrils with a K_d_ value of 20.7 nM. [^18^F]THK523 was bound to tau neurofibrillary tangles but not to β-amyloid plaques in the hippocampus of post-mortem AD brain slices as visualized with in vitro autoradiography and immunostaining studies.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=THK523%20and%20rodentia)]

Fodero-Tavoletti et al. (16) performed ex vivo biodistribution studies of [^18^F]THK523 (0.68–1.32 MBq (18–36 μCi)) after intravenous injection into normal male mice (n = 4/group) at 2, 10, 30, and 60 min after injection. [^18^F]THK523 showed an initial rapid penetration into the brain with 2.75% injected dose (ID)/g at 2 min, with a quick washout (1.5% ID/g at 60 min). The organs with high accumulation at 2 min after injection were the kidney (~6.2% ID/g), heart (~6.2% ID/g), and liver (~5% ID/g), and all of these organs exhibited a fast clearance. Accumulation in the intestine was ~2% ID/g at 2 min and increased to 10% ID/g at 60 min, suggesting elimination of [^18^F]THK523 through biliary excretion. The radioactivity levels at 60 min were 1.7% and 2.0% in the blood and bone, respectively.

Fodero-Tavoletti et al. (16) performed PET imaging over 30 minutes in tau transgenic mice (rTg4510, n = 8) and wild-type mice (CamKII, n = 7) after injection of 3.7 MBq (0.1 mCi) [^18^F]THK523. [^18^F]THK523 showed an initial rapid penetration into the brain of rTg4510 mice with 4% ID/g at 2 min, with a quick washout (1.3% ID/g at 30 min). The accumulation of [^18^F]THK523 in the brain of wild-type mice at 30 min after injection was 48% lower (P < 0.007) than that in the brain of rTg4510 mice at the same time point. The accumulation levels of [^18^F]THK523 in the liver, intestine, and bone were similar in both types of mice. [^18^F]THK523 PET imaging over 30 minutes was next performed in APP/PS1 transgenic mice (n = 3) and their wild-type littermates (n = 3). There was no difference in retention in the brains of APP/PS1 and wild-type mice. The retention was significantly lower than that of rTg4510 mice (P < 0.0001). Immunohistological analysis showed colocalization of radioactivity with tau deposits in the brain sections of rTg4510 mice but not with β-amyloid plaques in the brain sections of APP/PS1 mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=THK523%20and%20%28dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=THK523%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=THK523%20and%20humans)]

No publication is currently available.

## References

1 Forstl H., Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
2 Heininger K. (2000). A unifying hypothesis of Alzheimer's disease. IV. Causation and sequence of events. Rev Neurosci.
3 Hardy J.A., Higgins G.A. (1992). Alzheimer's disease: the amyloid cascade hypothesis. Science.
4 Mirra S.S., Heyman A., McKeel D., Sumi S.M., Crain B.J., Brownlee L.M., Vogel F.S., Hughes J.P., van Belle G., Berg L. (1991). The Consortium to Establish a Registry for Alzheimer's Disease (CERAD). Part II. Standardization of the neuropathologic assessment of Alzheimer's disease. Neurology.
5 Brandt R., Hundelt M., Shahani N. (2005). Tau alteration and neuronal degeneration in tauopathies: mechanisms and models. Biochim Biophys Acta.
6 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
7 de Leon M.J., DeSanti S., Zinkowski R., Mehta P.D., Pratico D., Segal S., Clark C., Kerkman D., DeBernardis J., Li J., Lair L., Reisberg B., Tsui W., Rusinek H. (2004). MRI and CSF studies in the early diagnosis of Alzheimer's disease. J Intern Med.
8 Bacskai B.J., Klunk W.E., Mathis C.A., Hyman B.T. (2002). Imaging amyloid-beta deposits in vivo. J Cereb Blood Flow Metab.
9 Klunk W.E., Engler H., Nordberg A., Bacskai B.J., Wang Y., Price J.C., Bergstrom M., Hyman B.T., Langstrom B., Mathis C.A. (2003). Imaging the pathology of Alzheimer's disease: amyloid-imaging with positron emission tomography. Neuroimaging Clin N Am.
10 Klunk W.E., Engler H., Nordberg A., Wang Y., Blomqvist G., Holt D.P., Bergstrom M., Savitcheva I., Huang G.F., Estrada S., Ausen B., Debnath M.L., Barletta J., Price J.C., Sandell J., Lopresti B.J., Wall A., Koivisto P., Antoni G., Mathis C.A., Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.
11 Kung M.P., Hou C., Zhuang Z.P., Skovronsky D., Kung H.F. (2004). Binding of two potential imaging agents targeting amyloid plaques in postmortem brain tissues of patients with Alzheimer's disease. Brain Res.
12 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
13 Wang Y., Klunk W.E., Debnath M.L., Huang G.F., Holt D.P., Shao L., Mathis C.A. (2004). Development of a PET/SPECT agent for amyloid imaging in Alzheimer's disease. J Mol Neurosci.
14 Shoghi-Jadid K., Small G.W., Agdeppa E.D., Kepe V., Ercoli L.M., Siddarth P., Read S., Satyamurthy N., Petric A., Huang S.C., Barrio J.R. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
15 Okamura N., Suemoto T., Furumoto S., Suzuki M., Shimadzu H., Akatsu H., Yamamoto T., Fujiwara H., Nemoto M., Maruyama M., Arai H., Yanai K., Sawada T., Kudo Y. (2005). Quinoline and benzimidazole derivatives: candidate probes for in vivo imaging of tau pathology in Alzheimer's disease. J Neurosci.
16 Fodero-Tavoletti M.T., Okamura N., Furumoto S., Mulligan R.S., Connor A.R., McLean C.A., Cao D., Rigopoulos A., Cartwright G.A., O'Keefe G., Gong S., Adlard P.A., Barnham K.J., Rowe C.C., Masters C.L., Kudo Y., Cappai R., Yanai K., Villemagne V.L. (2011). 18F-THK523: a novel in vivo tau imaging ligand for Alzheimer's disease. Brain.